# [^18^F]5-(6-Fluorohexyn-1-yl)-3-[2(S)-2-azetidinylmethoxy]pyridine

Chemical name: | [^18^F]5-(6-fluorohexyn-1-yl)-3-[2(S)-2-azetidinylmethoxy]pyridine
Abbreviated name: | [^18^F]ZW-104
Synonym:
Agent category: | Compound
Target: | Neuronal α4β2 nicotinic acetylcholine receptor (nAChR)
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Other Non-primate Mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ZW-104)]

Neuronal α4β2 nicotinic cholinergic receptors (nAChRs) are part of a heterogeneous family of ligand-gated ion channels expressed in the central nervous system, where their activation by acetylcholine and nicotine causes a rapid increase in cellular permeability to ions such as Na^+^ and Ca^2+^ (1-3). Nicotinic receptors exist as pentamers (homomeric or heteromeric) in various brain regions and ganglia. There are nine subtypes of ligand-binding α receptors (α2 to α10) and four subtypes of structural β receptors (β2 to β5). nAChRs have been found to be involved in cognitive processes such as learning, memory, and control of movement in normal subjects. nAChR dysfunction has been implicated in a number of human diseases such as schizophrenia, Huntington's disease, Alzheimer's disease, and Parkinson's disease. nAChRs also play a significant role in nicotine addiction and other health problems associated with tobacco smoking.

3-[2(S)-2-Azetidinylmethoxy]pyridine (A-85380) is a highly potent and selective α4β2 nAChR agonist with subnanomolar affinity (4, 5). 6-[^18^F]Fluoro-A-85380 and 2-[^18^F]fluoro-A-85380 have been studied in humans as positron emission tomography (PET) agents for α4β2 nAChR imaging in the brain. A-85380 has also been labeled as 5-[^123^I]iodo-A-85380 (5-[^123^I]IA), which has been developed as a single-photon emission computed tomography (SPECT) agent for the noninvasive study of α4β2 nAChR in the brain. However, prolonged imaging times (>5 h) are required for reliable quantification because of the slow kinetics of this agent. 5-(6-Hydroxyhexyn-1-yl)-A-85380 (sazetidine-A), a derivative of A-85380, has been shown to be a potent and selective β2 nAChR agonist for α4β2 nAChR with subnanomolar affinity (6). [^18^F]5-(6-Fluorohexyn-1-yl)-A-85380 ([^18^F]ZW-104) is being developed as a PET agent for the noninvasive study of α4β2 nAChR in the brain (7).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=nAChR+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (nAChR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=1137)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=Neuronal%5BAll+Fields%5D+AND+nicotinic%5BAll+Fields%5D+AND+acetylcholine%5BAll+Fields%5D+AND+receptor%5BAll+Fields%5D)
- Clinical trials (nAChR (http://www.clinicaltrials.gov/ct2/results?term=nAChR))
- Drug information in FDA (http://google2.fda.gov/search?q=Neuronal+nicotinic+acetylcholine+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14)
- Information about [^18^F]ZW-104 in PubChem (http://www.ncbi.nlm.nih.gov/sites/entrez?cmd=search&db=pcsubstance&term=85752742%5buid%5d)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ZW-104%20and%20synthesis)]

Valette et al. (7) reported synthesis of [^18^F]ZW-104 by the standard ([^18^F]KF/Kryptofix 2.2.2) ^18^F-nucleophilic aromatic fluorination of the corresponding N-Boc–protected tosyloxy precursor for 8 min at 120ºC. The N-Boc–protected [^18^F]ZW-104 was hydrolyzed with trifluoroacetic acid and purified with high-performance liquid chromatography (HPLC). Radiochemical yields were 3–5% at the end of synthesis. The radiochemical purity was >99% with specific activities of 37–74 GBq/µmol (1–2 Ci/µmol) at the end of synthesis. The total synthesis time was 100 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ZW-104%20and%20in%20vitro)]

Valette et al. (7) reported that ZW-104 exhibited inhibition constant (K_i_) values of 0.8, 200, 0.64, 5,500, 0.2, and 120 nM in human α2β2, α2β4, α3β2, α3β4, α4β2, and α4β4 receptors labeled with [^3^H]epibatidine, respectively. In comarision, 2-fluoro-A-85380 exhibited K_i_ values of 1.44, 181, 3.02, 3,600, 1.33, and 24 nM in human α2β2, α2β4, α3β2, α3β4, α4β2, and α4β4 receptors labeled with [^3^H]epibatidine, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ZW-104%20and%20rodentia)]

Vallette et al. (7) reported that the fractions of unchanged [^18^F]ZW-104 in rat plasma and brain, at 70 min after injection as determined with HPLC were 17.5% and >99%, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ZW-104%20and%20(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ZW-104%20and%20(primate%20not%20human))]

PET studies with five baboons showed substantial brain accumulation with selective maximal uptake (SUV_max_) of 5.7 in the thalamus at 35–50 min after injection of 152 MBq (4.1 mCi, 6.3 nmol) [^18^F]ZW-104 and intermediate uptake in the cortex and basal ganglia (~4.0) at 50–60 min after injection (7). The cerebellum (SUV_max_, 2.8 at 35 min) showed lower binding than the other brain regions, whereas it exhibited a faster washout rate than that of all other regions measured. Logan analysis showed that 30, 45, and 55 min were necessary for the volume of distribution to become time-invariant in the cerebellum, frontal cortex, and thalamus, respectively. The thalamus/cerebellum volume of distribution ratio was 3.5 at 180 min and 360 min. [^18^F]ZW-104 radioactivity was reduced to background level of cerebellum by pretreatment with nicotine or ZW-104 (2,500 nmol/kg, 30 min). Whole-body imaging showed a high accumulation of radioactivity in the kidney, urinary bladder, gallbladder, and intestines at 185 min after injection. Bone radioactivity was low. The fraction of unchanged [^18^F]ZW-104 in the plasma as determined with HPLC was 64%, 50%, and 32% at 30, 50, and 120 min after injection, respectively. Five labeled metabolites were found; their lipophilicity was not determined. Distribution volume values in different brain regions were two-fold higher for [^18^F]ZW-104 than for 2-[^18^F]fluoro-A-85380, and the occurrence of peak uptake in the thalamus (~35 min after injection) was earlier than that of 2-[^18^F]fluoro-A-85380 (>60 min after injection).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ZW-104%20and%20human)]

No publication is currently available.

## References

1 Alkondon M., Albuquerque E.X. (2004). The nicotinic acetylcholine receptor subtypes and their function in the hippocampus and cerebral cortex. Prog Brain Res.
2 Gotti C., Riganti L., Vailati S., Clementi F. (2006). Brain neuronal nicotinic receptors as new targets for drug discovery. Curr Pharm Des.
3 Hogg R.C., Raggenbass M., Bertrand D. (2003). Nicotinic acetylcholine receptors: from structure to brain function. Rev Physiol Biochem Pharmacol.
4 Abreo M.A., Lin N.H., Garvey D.S., Gunn D.E., Hettinger A.M., Wasicak J.T., Pavlik P.A., Martin Y.C., Donnelly-roberts D.L., Anderson D.J., Sullivan J.P., Williams M., Arneric S.P., Holladay M.W. (1996). Novel 3-Pyridyl ethers with subnanomolar affinity for central neuronal nicotinic acetylcholine receptors. J Med Chem.
5 Sullivan J.P., Donnelly-Roberts D., Briggs C.A., Anderson D.J., Gopalakrishnan M., Piattoni-Kaplan M., Campbell J.E., McKenna D.G., Molinari E., Hettinger A.M., Garvey D.S., Wasicak J.T., Holladay M.W., Williams M., Arneric S.P. (1996). A-85380 [3-(2(S)-azetidinylmethoxy) pyridine]: in vitro pharmacological properties of a novel, high affinity alpha 4 beta 2 nicotinic acetylcholine receptor ligand. Neuropharmacology.
6 Zwart R., Carbone A.L., Moroni M., Bermudez I., Mogg A.J., Folly E.A., Broad L.M., Williams A.C., Zhang D., Ding C., Heinz B.A., Sher E. (2008). Sazetidine-A is a potent and selective agonist at native and recombinant alpha 4 beta 2 nicotinic acetylcholine receptors. Mol Pharmacol.
7 Valette H., Xiao Y., Peyronneau M.A., Damont A., Kozikowski A.P., Wei Z.L., Kassiou M., Kellar K.J., Dolle F., Bottlaender M. (2009). 18F-ZW-104: a new radioligand for imaging neuronal nicotinic acetylcholine receptors--in vitro binding properties and PET studies in baboons. J Nucl Med.